# Poly(ethylene glycol)-coated gold nanocages

Chemical name: | Poly(ethylene glycol)-coated gold nanocages
Abbreviated name: | PEG-AuNCs
Synonym:
Agent category: | Metal
Target: | Non-targeted
Target category: | Non-targeted
Method of detection: | Ultrasound, photoacoustic tomography (PAT) imaging
Source of signal: | Gold (Au)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanocages)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a noninvasive alternative to radionuclide imaging in small animals (4, 5).

Photoacoustic imaging (PAI) is an emerging hybrid biomedical imaging modality based on the photoacoustic effect. In PAI, non-ionizing optical pulses are delivered into biological tissues. Some of the delivered energy is absorbed and converted into heat, leading to transient thermoelastic expansion and thus ultrasonic emission. The generated ultrasonic waves are then detected by ultrasonic transducers to form images. It is known that optical absorption is closely associated with physiological properties, such as hemoglobin concentration and oxygen saturation. As a result, the magnitude of the ultrasonic emission (i.e., the photoacoustic signal), which is proportional to the local energy deposition, reveals physiologically specific optical absorption contrast and tissue structures. However, exogenous NIR contrast agents are necessary to overcome the intrinsic low tissue- and hemoglobin-absorption and scattering of tissue. On the other hand, these small molecules exhibit fast clearance, small optical absorption cross section, and non-targeted specificity. Therefore, there is a need for contrast agents with long blood circulation and targeted specificity.

Gold (Au) nanoparticles have been studied as molecular imaging agents because of their bright NIR fluorescence emission around 700–900 nm and low toxicity (6, 7). They can be tuned to emit in a range of wavelengths by changing their sizes, shapes, and composition, thus providing broad excitation profiles and high absorption coefficients. They can be coated and capped with hydrophilic materials for additional conjugation with biomolecules, such as peptides, antibodies, nucleic acids, and small organic compounds for in vitro and in vivo studies. Au nanoparticles have been approved by the United States Food and Drug Administration for treatment of patients with rheumatoid arthritis. Au nanoparticles have been studied as contrast agents in X-ray/computed tomography, NIR optical coherence tomography, PAI, and photoacoustic tomography (PAT) (8). NIR Au nanocages (AuNCs) are biocompatible, have low toxicity, and are tunable to strong NIR absorption (9). They have an outer edge of ~50 nm and an inner edge of ~42 nm, with a wall thickness of ~4 nm. Yang et al. (10) performed PAT of the cerebral cortex of rats with poly(ethylene glycol)-coated AuNCs (PEG-AuNCs) as the optical contrast agent. The investigators observed an enhanced optical contrast in the vasculature in the cerebral cortex.

### Related Resource Links:

- Chapters in MICAD (Gold imaging (http://www.ncbi.nlm.nih.gov/books?term=Gold%20AND%20micad%5Bbook%5D))
- Clinical trials (Gold nanoparticles (http://www.clinicaltrials.gov/ct2/results?term=gold+AND+nanoparticles))
- Drug information in FDA (Gold nanoparticles (http://google2.fda.gov/search?q=gold%2BAND%2Brheumatoid%2Barthritis&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanocages%20and%20synthesis)]

Yang et al. (10) reported the synthesis of PEG-AuNCs by addition of 5.4 ml HAuCl_4_ (0.5 mM) to a 10 ml aqueous solution of Ag nanocubes containing poly(vinyl pyrrolidone) (PVP, 0.1 mg/ml) with stirring for 10 min at 100ºC. Upon cooling to room temperature, excess NaCl was added to remove Ag as AgCl. The supernatant was discarded, and AuNCs were resuspended in water. The AuNC alloy was composed of 70% Au and 30% Ag. AuNCs were washed six times to remove PVP and NaCl. AuNC surfaces were functionalized with PEG by adding 1 mL of a 1-mM PEG-SH (5 kDa) to a 2-nM AuNC suspension. The suspension was gently agitated and then allowed to sit undisturbed overnight. Residual PEG-SH was removed by centrifugation.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanocages%20and%20in%20vitro)]

PEG-AuNCs have a maximum optical absorption at 820 nm (10). PEG-AuNCs have an outer edge of ~50 nm and an inner edge of ~42 nm, with a wall thickness of ~4 nm as estimated with scanning electron microscopy and transmission electron microscopy.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanocages%20and%20rodentia)]

Yang et al. (10) performed noninvasive PAT of one rat brain after intravenous injection of a single dose of 0.8 × 10^9^ PEG-AuNCs/g body weight or three successive doses of 0.8 × 10^9^ PEG-AuNCs/g. PAT scanning began immediately after injection and continued for ~3 h with the laser wavelength at 804 nm. PAT images revealed a greater optical contrast after injection with PEG-AuNCs compared with PAT imaging before injection. There was a gradual enhancement of the optical absorption in the vasculature of the cerebral cortex, with a peak value of 81% at ~2 h after the third injection. There was a gradual decrease in absorption to 40% enhancement at 6 h. In another rat with a single-dose injection, there was a peak value of 35% enhancement at ~2 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanocages%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanocages%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanocages%20and%20human)]

No publication is currently available.

## NIH Support

R01 NS46214, R01 EB000712, 5DP1 OD000798

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Vosch T., Antoku Y., Hsiang J.C., Richards C.I., Gonzalez J.I., Dickson R.M. (2007). Strongly emissive individual DNA-encapsulated Ag nanoclusters as single-molecule fluorophores. Proc Natl Acad Sci U S A.
7 Chithrani B.D., Ghazani A.A., Chan W.C. (2006). Determining the size and shape dependence of gold nanoparticle uptake into mammalian cells. Nano Lett.
8 Choi H.S., Frangioni J.V. (2010). Nanoparticles for biomedical imaging: fundamentals of clinical translation. Mol Imaging.
9 Yang X., Stein E.W., Ashkenazi S., Wang L.V. (2009). Nanoparticles for photoacoustic imaging. Wiley Interdiscip Rev Nanomed Nanobiotechnol.
10 Yang X., Skrabalak S.E., Li Z.Y., Xia Y., Wang L.V. (2007). Photoacoustic tomography of a rat cerebral cortex in vivo with au nanocages as an optical contrast agent. Nano Lett.